# 2-(1-{6-[(2-[^18^F]Fluoroethyl)(methyl)amino]-2-naphthyl}ethylidene)malononitrile

Chemical name: | 2-(1-{6-[(2-[^18^F]Fluoroethyl)(methyl)amino]-2-naphthyl}ethylidene)malononitrile
Abbreviated name: | [^18^F]FDDNP
Synonym:
Agent Category: | Compound
Target: | Aggregates of amyloid-beta peptide and tangles tau protein
Target Category: | Acceptor
Method of detection: | PET
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDDNP%5BAll%20Fields%5D)]

Alzheimer's disease (AD) is a form of dementia with a gradual memory loss and a progressive decline in mental functions overtime (1, 2). It is characterized pathologically by neuronal loss, extracellular senile plaques (SPs; aggregates of amyloid-beta peptides consisting of 40 to 42 amino acids) and intracellular neurofibrillary tangles (NFTs; filaments of microtubule-binding hyper-phosphorylated protein tau) in the brain, especially in the hippocampus and associative regions of the cortex (3, 4). Beta-amyloid peptides and tau protein are implicated as the main causes of neuronal degeneration and cell death (5, 6).

Early diagnosis of AD is important for treatment consideration and disease management. Various β-amyloid imaging agents have been developed for magnetic resonance imaging (MRI), single photon emission computed tomography (SPECT), and positron emission tomography (PET) (7-12). The binding of different derivatives of Congo red, thioflavin, stibene, and aminonaphthalene has been studied in human post-mortem brain tissue and in transgenic mice. Out of these analogues, N-methyl-[^11^C]-2-(4’-methylaminophenyl)-6-hydroxybenzothiasole, a amyloid-beta binding compound based on a series of neutral thioflavin-T derivatives (13), was radiolabeled with the positron-emitting radionuclide ^11^C ([^11^C]6-OH-BTA-1 or [^11^C]PIB). [^11^C]6-OH-BTA-1 was found to be a promising imaging agent for the senile plaques in the brain (9). On the other hand, 2-(1-(6-[(2-[^18^F]fluoroethyl)(methyl)amino]-2-naphthyl)ethylidene)malono nitrile ([^18^F]FDDNP) was studied in humans, showing more binding in the brains of patients with AD than in those of healthy people (14). Despite of its slow clearance kinetics for PET imaging, [^18^F]FDDNP has been found to be a useful tool for detection of both neurofibrillary tangles (NFTs) and amyloid-beta senile plaques (APs) in AD patients.

### Related Resource Links:

- Chapters in MICAD (Amyloid (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=amyloid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Amyloid (http://www.ncbi.nlm.nih.gov/gene/351)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amyloid (http://www.ncbi.nlm.nih.gov/omim/?term=Amyloid))
- Clinical trials (Amyloid (http://www.clinicaltrials.gov/ct2/results?term=Amyloid), [^18^F]FDDNP (http://www.clinicaltrials.gov/ct2/results?term=18F+FDDNP))
- Drug information in FDA (Amyloid inhibitors (http://google2.fda.gov/search?q=Amyloid+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=16&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDDNP%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

The Bucherer reaction of 1-(6-hydroxy-2-naphthyl)-1-ethanone with 2-(methylamino)ethanol yielded 1-{6-[(2-hydroxyethyl)(methyl) amino]-2-naphthyl}-1-ethanone. The Knoevenagel reaction of the Bucherer product with malononitrile yielded 2-1-{6-[(2-hydroxyethyl)(methyl)amino]-2-naphthyl}ethylidene malononitrile, which upon reaction with 4-methylbenzenesulfonyl anhydride (14), resulted in the sulfonated precursor. Reaction of the precursor with K[^18^F]F/Kryptofix 222 yielded [^18^F]FDDNP. After purification by high-performance liquid chromatography (HPLC), radiochemically and chemically pure [^18^F]FDDNP was prepared in 10-20% radiochemical yield (end-of-synthesis) in a synthesis time of 90 min with specific activity of 222-999 GBq/μmol (6-27 Ci/μmol). Another method was to use p-toluenesulfonyl chloride (15) to form the tosylated precursor for K[^18^F]F/Kryptofix 222 fluorination to give 11% radiochemical yield at the end-of-synthesis in a total synthesis time of 90 min. The specific activity was 74-222 GBq/μmol (2-6 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDDNP%5BAll%20Fields%5D%20AND%20%28%22in%20vitro%22%5BMeSH%20Terms%5D%20OR%20in%20vitro%5BText%20Word%5D%29)]

Agdeppa et al. (16) reported that unlabeled FDDNP binds to aggregated amyloid-beta(1-40) fibrils with two affinities with K_d_ values of 0.16 and 1.86 nM. The B_max_ values are 80.8 and 164 pmol/mg for the high affinity and low affinity binding sites, respectively. Saturation binding studies with [^18^F]FDDNP to homogenates of frontal cortex from postmortem AD brain showed a K_d_ value of 0.74 nM and a B_max_ value of 144 nmol/g tissue. There was no specific binding of [^18^F]FDDNP to homogenates of frontal cortex from age-matched control brain.

Confocal fluorescence microscopy and digital autoradiography revealed that [^18^F]FDDNP is binding to both SPs and NFTs in the temporal and parietal cortices of AD patients (15). Their localizations were confirmed using antibodies to tau and amyloid-beta. Both white and gray matter of the same patient brain slices showed low background. FDDNP is able to cross the blood-brain barrier and the cellular membranes of neurons because it is highly lipophilic. Therefore, [^18^F]FDDNP is able to detect both SPs and NFTs in AD brains.

Another interesting finding was that non-steroidal anti-inflammatory drugs (NSAIDs), such as naproxen and ibuprofen, inhibited [^18^F]FDDNP binding to synthetic amyloid-beta(1-40) aggregates (17). The Ki values were 2.6 nM for (R)-naproxen, 5.7 nM for (S)-naproxen, 44.4 μM for (R)-ibuprofen and 11.3 μM for (S)-ibuprofen. Naproxen and ibuprofen also blocked the [^18^F]FDDNP binding sites on AD brain slices. Furthermore, FDDNP, naproxen and ibuprofen induced dissolution of aggregated amyloid-beta(1-40) fibrils. Diclofenac (another NSAID), Congo Red, and thioflavine did not show any inhibition of FDDNP specific binding in both the amyloid-beta(1-40) binding and anti-aggregation assays. An NSAID, such as naproxen is able to bind to SPs in AD and may act as anti-aggregation agent. NSIADs may be useful in therapeutic treatment of AD. The binding sites of FDDNP to amyloid-beta(1-40) aggregates were postulated to be different from those of Congo Red and thioflavine-S, which were tested up 1 μM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDDNP%5BAll%20Fields%5D%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20rodentia%5BText%20Word%5D%29)]

Teng et al. (18) performed [^18^F]FDDNP PET imaging in a transgenic rat model of AD to measure [^18^F]FDDNP binding profiles in relation to age-associated accumulation of amyloid-beta plaques. Cross-section [^18^F]FDDNP images were obtained transgenic rats (n = 3/group) and wild-type rats (n = 2-4/group) ranging from 9 to 22 months of age. [^18^F]FDDNP standard update value ratio (SUVR, cerebellium as reference) values increased with age in the hippocampus and frontal cortex of transgenic rats (P < 0.001). These values were significantly higher than those in age-matched wild-type rats (P < 0.05). The hippocampal and frontal SUVR values of transgenic rats were 1.09-1.12, 1.15, and 1.21 at 9, 14 and 20 months of age, whereas those (<1.08) of wild-type rats remained stable with age. Biochemical and Immunohistochemical analyses showed that the age-related changes in [^18^F]FDDNP binding in the the hippocampus and frontal cortex of transgenic rats paralleled the age-related changes in amyloid-beta levels as measured with an antibody against synthetic peptide amyloid-beta_1-13_ but not with thioflavine-S. Blocking studies (naproxen pretreatment) were performed with 17-month-old transgenic rats (n = 5) and 14-month-old wild-type rats (n = 2). Naproxen pretreatment decreased [^18^F]FDDNP SUVR values in the hippocampus and frontal cortex from 1.18 to 1.11 (P < 0.05). The SUVR values returned to 1.17 after naproxen washout. Little changes in the SUVR values (1.08) were observed in the wild-type rats with naproxen blockade.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDDNP%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDDNP%20and%20primate%20not%20human)]

Noda et al. (19) compared [^18^F]FDDNP and [^11^C]PIB brain accumulation on five aged and five young adult male rhesus macaques using PET. Both tracers showed increased accumulation in the striatum, thalamus, cingulate and pons in the aged group. Compared to [^11^C]PIB, [^18^F]FDDNP showed higher accumulation in the cortical regions of aged and young monkeys. [^18^F]FDDNP exhibited a higher non-specific binding than [^11^C]PIB.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDDNP%5BAll%20Fields%5D%20AND%20%28%22humans%22%5BMeSH%20Terms%5D%20OR%20humans%5BText%20Word%5D%29)]

The first human study with [^18^F]FDDNP PET in 9 patients with early AD and 7 healthy people was reported by Shoghi-Jadid et al. (14). The subjects were given an intravenous injection of 185-370 MBq (5-10 mCi) of [^18^F]FDDNP. The dynamic PET scans showed that [^18^F]FDDNP retention averaged 1.87 fold greater in brain regions (such as frontal, parietal, temporal, and occipital cortex, and hippocampus) that are known to contain APs and NFTs in AD patients than controls. The hippocampus had the highest relative residence time (RRT) of 8.13 min. There was low retention of [^18^F]FDDNP in the pons with little AP and NFT deposits in AD and controls. There is a direct correlation of RRT with mini-mental state exam scores (r_s_ = -0.87, p<0.0001; n = 16). There is an inverse correlation of [^18^F]FDDNP retention with low brain FDG metabolism and MRI atrophy in the cortical regions. Internal dosimetry data for [^18^F]FDDNP in humans is not available in the literature.

Tolboom et al. (20) performed paired [^11^C]PIB and [^18^F]FDDNP PET scans in 14 patients with AD, 11 patients with amnestic mild cognitive impairment (MCI), and 13 healty controls. Global cortical binding potential (BP_ND_) of [^11^C]PIB showed higher binding in patients with AD than in controls and MCI patients. [^18^F]FDDNP uptake was higher in AD patients than in controls, but MCI could not be distinguished from AD or from controls. Global BP_ND_ values of both tracers were moderately correlated (r = 0.45; P = 0.005). In MCI, BP_ND_ of [^11^C]PIB showed a bimodal distribution, whereas BP_ND_ values for [^18^F]FDDNP were more widespread, with more MCI patients demonstrating increased accumulation. Regional [^11^C]PIB BP_ND_ showed different patterns across diagnostic groups, as AD patients showed an overall increase in binding, with the lowest binding in the medial temporal lobe. With [^18^F]FDDNP, patterns were similar across diagnostic groups. For all groups, highest BP_ND_ values were observed in the medial temporal lobe. Differences in BP_ND_ values between patients with AD, patients with MCI, and controls were more pronounced for [^11^C]PIB. The difference in regional binding, the moderate correlation, and the discrepant findings in MCI suggest that they measure related, but different, characteristics of the disease. In another study, Tolboom et al. (21) showed that increased [^18^F]FDDNP binding was associated with impairment of episodic memory, whereas [^11^C]PIB binding was associated with impairment in a broader range of cognitive functions.

## NIH Support

P50 AG16570, K08 AG34628, P01 AG025831

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci.
3 Hardy J.A., Higgins G.A. (1992). Alzheimer's disease: the amyloid cascade hypothesis. Science.
4 Mirra S.S., Heyman A., McKeel D., Sumi S.M., Crain B.J., Brownlee L.M., Vogel F.S., Hughes J.P., van Belle G., Berg L. (1991). The Consortium to Establish a Registry for Alzheimer's Disease (CERAD). Part II. Standardization of the neuropathologic assessment of Alzheimer's disease. Neurology.
5 Brandt R., Hundelt M., Shahani N. (2005). Tau alteration and neuronal degeneration in tauopathies: mechanisms and models. Biochim Biophys Acta.
6 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
7 Bacskai B.J., Klunk W.E., Mathis C.A., Hyman B.T. (2002). Imaging amyloid-beta deposits in vivo. J Cereb Blood Flow Metab.
8 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
9 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
10 Klunk W.E., Engler H., Nordberg A., Bacskai B.J., Wang Y., Price J.C., Bergstrom M., Hyman B.T., Langstrom B., Mathis C.A. (2003). Imaging the pathology of Alzheimer's disease: amyloid-imaging with positron emission tomography. Neuroimaging Clin N Am.
11 Wang Y., Klunk W.E., Debnath M.L., Huang G.F., Holt D.P., Shao L., Mathis C.A. (2004). Development of a PET/SPECT agent for amyloid imaging in Alzheimer's disease. J Mol Neurosci.
12 Kung M.P., Hou C., Zhuang Z.P., Skovronsky D., Kung H.F. (2004). Binding of two potential imaging agents targeting amyloid plaques in postmortem brain tissues of patients with Alzheimer's disease. Brain Res.
13 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
14 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
15 Agdeppa E.D., Kepe V., Liu J., Small G.W., Huang S.C., Petric A., Satyamurthy N., Barrio J.R. (2003). 2-Dialkylamino-6-acylmalononitrile substituted naphthalenes (DDNP analogs): novel diagnostic and therapeutic tools in Alzheimer's disease. Mol Imaging Biol.
16 Agdeppa E.D., Kepe V., Liu J., Flores-Torres S., Satyamurthy N., Petric A., Cole G.M., Small G.W., Huang S.C., Barrio J.R. (2001). Binding characteristics of radiofluorinated 6-dialkylamino-2-naphthylethylidene derivatives as positron emission tomography imaging probes for beta-amyloid plaques in Alzheimer's disease. J Neurosci.
17 Agdeppa E.D., Kepe V., Petri A., Satyamurthy N., Liu J., Huang S.C., Small G.W., Cole G.M., Barrio J.R. (2003). In vitro detection of (S)-naproxen and ibuprofen binding to plaques in the Alzheimer's brain using the positron emission tomography molecular imaging probe 2-(1-[6-[(2-[(18)F]fluoroethyl)(methyl)amino]-2-naphthyl]ethylidene)malono nitrile. Neuroscience.
18 Teng, E., V. Kepe, S.A. Frautschy, J. Liu, N. Satyamurthy, F. Yang, P.P. Chen, G.B. Cole, M.R. Jones, S.C. Huang, D.G. Flood, S.P. Trusko, G.W. Small, G.M. Cole, and J.R. Barrio, [F-18]FDDNP microPET imaging correlates with brain Abeta burden in a transgenic rat model of Alzheimer disease: Effects of aging, in vivo blockade, and anti-Abeta antibody treatment. Neurobiol Dis, 2011
19 Noda A., Murakami Y., Nishiyama S., Fukumoto D., Miyoshi S., Tsukada H., Nishimura S. (2008). Amyloid imaging in aged and young macaques with [11C]PIB and [18F]FDDNP. Synapse.
20 Tolboom N., Yaqub M., van der Flier W.M., Boellaard R., Luurtsema G., Windhorst A.D., Barkhof F., Scheltens P., Lammertsma A.A., van Berckel B.N. (2009). Detection of Alzheimer pathology in vivo using both 11C-PIB and 18F-FDDNP PET. J Nucl Med.
21 Tolboom N., van der Flier W.M., Yaqub M., Koene T., Boellaard R., Windhorst A.D., Scheltens P., Lammertsma A.A., van Berckel B.N. (2009). Differential association of [11C]PIB and [18F]FDDNP binding with cognitive impairment. Neurology.